# ^99m^Tc-Labeled (1S,3S)-3-acetyl-1,2,3,4,6,11-hexahydro-3,5,12-trihydroxy-10-methoxy-6,11-dioxo-1-naphthacenyl 3-amino-2,3,6-trideoxy-α-L-lyxo-hexopyranoside

Chemical name: | ^99m^Tc-Labeled (1S,3S)-3-acetyl-1,2,3,4,6,11-hexahydro-3,5,12-trihydroxy-10-methoxy-6,11-dioxo-1-naphthacenyl 3-amino-2,3,6-trideoxy-α-L-lyxo-hexopyranoside
Abbreviated name: | [^99m^Tc]Daunorubicin
Synonym:
Agent Category: | Compound
Target: | DNA; DNA topoisomerase II alpha and beta
Target Category: | Nucleic acids; enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on structure of daunorubicin for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance). Binding site of ^99m^Tc not reported (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glycine%20transporter&cmd=DetailsSearch)]

Daunorubicin (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=29fe455e-f177-4b0e-99fb-60a53016db72), a member of the anthracycline family of antibiotics, is approved by the United States Food and Drug Administration (FDA) for the remission induction of acute nonlymphocytic leukemia in adults and for the remission induction of acute lymphocytic leukemia in children and adults. Anthracyclines are known to inhibit cancer cell proliferation by several mechanisms, but it is well established that these antibiotics intercalate between the nucleotides of DNA and RNA and interfere with the replication of these nucleic acids. In addition, anthracyclines inhibit the topoisomerase II group of enzymes that have an important role in DNA replication (2). Doxorubicin (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=102358dc-2109-4829-b333-b99417334e39), another anthracycline antibiotic with a structure and mechanism of action similar to that of daunorubicin, has been approved by the FDA for the treatment of several types of cancers, such as acute lymphoblastic leukemia, acute myeloblastic leukemia, Wilms' tumor, neuroblastoma, soft tissue and bone sarcomas, breast carcinoma, ovarian carcinoma, transitional cell bladder carcinoma, thyroid carcinoma, gastric carcinoma, Hodgkin's disease, malignant lymphoma, and bronchogenic carcinoma.

Several radiochemicals, such as [^99m^Tc]-methoxyisobutyl-isonitrile ([^99m^Tc]-MIBI), [^99m^]Tc-tetrofosmin, and [^18^F]-fluorodeoxyglucose ([^18^F]-FDG), are often used in the clinic with single-photon emission computed tomography (SPECT; for noninvasive imaging with [^99m^Tc]-MIBI and [^99m^]Tc-tetrofosmin) and positron emission tomography (for imaging with [^18^F]-FDG) to detect and monitor cancerous tumors. However, these tracers are of limited use for the detection and monitoring of neoplastic lesions because they often generate false-positive results, as detailed elsewhere (3). Transformed cells have a characteristically high proliferation rate and consequently exhibit a higher rate of DNA synthesis compared with the normal cells. Therefore, cells with an elevated rate of DNA synthesis would be expected to intercalate high levels of anthracycline antibiotics within the nucleic acid structure. Based on this assumption, Kumar et al. evaluated the use of ^99m^Tc-labeled doxorubicin for the noninvasive detection of tumors in mice, and the investigators showed that the tracer was probably suitable for visualization of the lesions with scintigraphy in the rodents (3). Faheem et al. investigated the biodistribution of ^99m^Tc-labeled daunorubicin ([^99m^Tc]-daunorubicin) in normal rats, and scintigraphy was used to study the biodistribution of this radiolabeled compound in a rabbit (1). Results obtained from studies performed with [^99m^Tc]-daunorubicin are presented in this chapter.

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=%28%22doxorubicin%22%5BAll%20Fields%5D%20OR%20%22doxorubicin%22%5BAll%20Fields%5D%29%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=daunorubicin&Search=Search) with daunorubicin

Daunorubicin in Gene Database (http://www.ncbi.nlm.nih.gov/gene?term=Daunorubicin)

Daunorubicin resistance in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=daunorubicin%20resistance&cmd=DetailsSearch)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28%22daunorubicin%22%5BMeSH%20Terms%5D%20OR%20%22daunorubicin%22%5BAll%20Fields%5D%29%20AND%20%28%22metabolism%22%5BMeSH%20Terms%5D%20OR%20%22metabolism%22%5BAll%20Fields%5D%20OR%20%22synthesis%22%5BAll%20Fields%5D%29&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]-daunorubicin is detailed by Faheem et al. (1). The labeling reaction was reported to have an efficiency of ~96% when it was allowed to proceed at room temperature for 10–20 min in the presence of 4 μg stannous chloride. The radiochemical yield, radiochemical purity, and specific activity of [^99m^Tc]-daunorubicin were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28%22daunorubicin%22%5BMeSH%20Terms%5D%20OR%20%22daunorubicin%22%5BAll%20Fields%5D%29%20AND%20%28%22in%20vitro%22%5BPublication%20Type%5D%20OR%20%22in%20vitro%22%5BAll%20Fields%5D%29&cmd=DetailsSearch)]

The partition coefficient of [^99m^Tc]-daunorubicin was ~1.7 as determined with a 1-octanol and phosphate buffer (pH 7.0–7.4) mixture (1).

The radiochemical showed very little degradation (~5.0%; as determined with high-performance liquid chromatography) when it was incubated with normal human serum for 24 h at 25°C (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28%28%22daunorubicin%22%5BMeSH%20Terms%5D%20OR%20%22daunorubicin%22%5BAll%20Fields%5D%29%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20%22rodentia%22%5BAll%20Fields%5D%29%29&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-daunorubicin was investigated in male Sprague-Dawley rats as described by Faheem et al. (1). The animals (n = 5 rats/time point) were injected with ~74 MBq (2 mCi) [^99m^Tc]-daunorubicin through the tail vein, and the rodents were euthanized at various time points ranging from 1 h postinjection (p.i.) to 24 h p.i. All organs of interest were subsequently removed from the euthanized animals, and the amount of radioactivity accumulated in the various tissues was determined. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). At 1 h p.i., maximum tracer uptake was detected in the kidneys (9.98 ± 1.23% ID/g), followed by urine, blood, brain, heart, lungs, and intestine (4.65 ± 0.72% ID/g, 1.52 ± 0.23% ID/g, 1.60 ± 0.33% ID/g, 1.09 ± 0.07% ID/g, 1.07 ± 0.09% ID/g, and 0.60 ± 0.11% ID/g, respectively). By 24 h p.i., maximum radioactivity was present in the urine, followed by intestine, kidneys, heart, brain, blood, and lungs (6.95 ± 1.53% ID/g, 3.6 ± 0.76% ID/g , 2.03 ± 0.67% ID/g, 0.54 ± 0.12% ID/g, 0.49 ± 0.04% ID/g, 0.45 ± 0.04% ID/g, and 0.01 ± 0.01% ID/g, respectively). This indicated that the tracer was excreted from the system primarily through the renal route.

The biodistribution of [^99m^Tc]-daunorubicin was also studied with scintigraphy in a normal rabbit (1). The animal was injected with 15 MBq (405 μCi) [^99m^Tc]-daunorubicin through the ear vein, and whole-body scintigraphic images of the rabbit were acquired at 1 h p.i., 4 h p.i., and 24 h p.i. Radioactivity (not quantified by the investigators) was faintly visible in the brain at 1 h p.i., and the amount of tracer in this organ increased and was clearly visible by 4 h p.i. The kidneys and urinary bladder were clearly visible in the animals at both 1 h p.i. and 4 h p.i. By 24 h p.i., the accumulation of label in the brain, kidneys, and urinary bladder had reduced to a level that was lower than that visible at 1 h p.i.

From these studies, the investigators concluded that [^99m^Tc]-daunorubicin may be a suitable tracer for imaging the brain in rodents, but they cautioned that more investigations are necessary to confirm this observation before [^99m^Tc]-daunorubicin can be used in the clinic for this purpose (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28-daunorubicin%5BAll%20Fields%5D%20AND%20Non-Primate%5BAll%20Fields%5D%20AND%20Mammals%5BAll%20Fields%5D%29&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28-daunorubicin%5BAll%20Fields%5D%20AND%20Non-Human%5BAll%20Fields%5D%20AND%20Primates%5BAll%20Fields%5D%29&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc%5BAll%20Fields%5D%20AND%20%28%28%22daunorubicin%22%5BMeSH%20Terms%5D%20OR%20%22daunorubicin%22%5BAll%20Fields%5D%29%20AND%20%28%22Hum%20Stud%22%5BJournal%5D%20OR%20%28%22human%22%5BAll%20Fields%5D%20AND%20%22studies%22%5BAll%20Fields%5D%29%20OR%20%22human%20studies%22%5BAll%20Fields%5D%29%29&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Faheem A.R., Bokhari T.H., Roohi S., Mushtaq A., Sohaib M. (2013). (99m)Tc-daunorubicin a potential brain imaging and theranostic agent: synthesis, quality control, characterization, biodistribution and scintigraphy. Nucl Med Biol.
2 Sawyer D.B., Peng X., Chen B., Pentassuglia L., Lim C.C. (2010). Mechanisms of anthracycline cardiac injury: can we identify strategies for cardioprotection?. Prog Cardiovasc Dis.
3 Kumar P., Singh B., Sharma S., Ghai A., Chuttani K., Mishra A.K., Dhawan D., Mittal B.R. (2012). Preclinical evaluation of [99m]Tc-labeled doxorubicin as a potential scintigraphic probe for tumor imaging. Cancer Biother Radiopharm.